# ^125^I-Labeled anti-epidermal growth factor receptor human Fab antibody fragment

Chemical name: | ^125^I-Labeled anti-epidermal growth factor receptor human Fab antibody fragment
Abbreviated name: | ^125^I-Fab
Synonym:
Agent category: | Antibody fragment, Fab
Target: | Epidermal growth factor receptor (EGFR), HER1/erbB-1
Target category: | Receptor
Method of detection: | Single-photon emission computed tomography (SPECT)
Source of signal: | ^125^I
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&val=54792098), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?val=NM_201282.1) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=Graphics&list_uids=1956) for more information about EGFR.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Fab%20EGFR)]

Epidermal growth factor (EGF) is a cytokine that comprises 53 amino acids (6.2 kDa) and is secreted by ectodermic cells, monocytes, kidneys, and duodenal glands (1). EGF stimulates growth of epidermal and epithelial cells. EGF and at least seven other growth factors and their transmembrane receptor kinases play important roles in cell proliferation, survival, adhesion, migration, and differentiation. The EGF receptor (EGFR) family consists of four transmembrane receptors: EGFR (HER1/erbB-1), HER2 (erbB-2/neu), HER3 (erbB-3), and HER4 (erbB-4) (2). HER1, HER3, and HER4 comprise three major functional domains: an extracellular ligand-binding domain, a hydrophobic transmembrane domain, and a cytoplasmic tyrosine kinase domain. No ligand has been clearly identified for HER2; however, HER2 can be activated as a result of ligand binding to other HER receptors with the formation of receptor homodimers and/or heterodimers (3). HER1 and HER2 are overexpressed on many solid tumor cells such as breast, non-small cell lung, head and neck, and colon cancers (4-6). The high levels of HER1 and HER2 expression on cancer cells are associated with a poor prognosis (7-10).

Cetuximab is a humanized IgG_1_ monoclonal antibody (mAb) against the extracellular domain of recombinant EGFR (11). Cetuximab was approved by the United States Food and Drug Administration (FDA) to treat patients with advanced colorectal cancer that has metastasized to other parts of the body. Various labeled cetuximab probes have been developed for imaging human breast cancer in small-animal tumor models (12-14). However, the pharmacokinetics of the intact radiolabeled mAb, with high liver uptake and slow blood elimination, are generally not ideal for imaging. Smaller antibody fragments, such as Fab or F(ab´)_2_, have better imaging pharmacokinetics because they are rapidly excreted by the kidneys. Wang et al. (15) generated a human Fab antibody fragment against the extracellular domain of EGFR from a human naive Fab phage library. Xu et al. (16) evaluated ^125^I-anti-EGFR human Fab antibody fragment (^125^I-Fab) for single-photon emission computed tomography (SPECT) imaging in nude mice bearing human EGFR-expressing tumors.

### Related Resource Links:

- Chapters in MICAD (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=books&Cmd=DetailsSearch&Term=EGFR+AND+micad%5Bbook%5D)
- Gene information in NCBI (EGFR (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=gene&Cmd=DetailsSearch&Term=1956))
- Articles in OMIM (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=omim&Cmd=DetailsSearch&Term=EGFR)
- Clinical trials (EGFR (http://www.clinicaltrials.gov/ct2/results?term=EGFR))
- FDA Drug information (EGFR (http://google2.fda.gov/search?q=EGFR&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=12&y=7))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Fab%20EGFR+synthesis)]

Anti-EGFR Fab (0.2 nmol) was labeled with 74 MBq (2 mCi) ^125^I in the presence of chloramine-T (16). ^125^I-Fab was isolated from the incubation mixture with a PD-10 column. The labeling efficiency was ~75%, and the radiochemical purity was >95%. ^125^I-Fab exhibited an immunoreactivity of 63%. The specific activity was not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Fab%20EGFR%20and%20in%20vitro)]

In vitro binding of Fab showed a binding affinity of 30 nM using noncompetitive radioimmunoassay (15). In vitro cell uptake assays were performed using three cell lines with different degree of EGFR expression (A431 > U118 > NIH3T3 cells) (16). The radioactivity levels were 120,000, 40,000, and 8,000 cpm in A431, U118, and NIH3T3 cells, respectively, at 1 h of incubation with 0.06 nM ^125^I-Fab. The radioactivity levels were reduced to 40,000, 20,000, and 7,000 cpm, respectively, by co-incubation with 1.2 nM anti-EGFR Fab.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Fab%20EGFR%20and%20rodentia)]

Whole-body gamma imaging analysis was performed in nude mice bearing A431, U118, or M14 tumors after intravenous injection of 11.1 MBq (300 μCi) ^125^I-Fab (16). The tumors (A431 > U118 > M14) and urinary bladder were clearly visualized at 15 h after injection. The tumor/muscle ratio was 15, 4, and 2 for A431, U118, and M14 tumors at 24 h after injection, respectively. No blocking experiment was performed. The use of low EGFR-expression tumors provided some specificity of ^125^I-Fab.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Fab%20EGFR%20and%20%28dog%20or%20pig%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Fab%20EGFR%20and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Fab%20EGFR%20and%20human)]

No publication is currently available.

## References

1 Carpenter G., Cohen S. (1990). Epidermal growth factor. J Biol Chem.
2 Yarden Y. (2001). The EGFR family and its ligands in human cancer. signalling mechanisms and therapeutic opportunities. Eur J Cancer.
3 Rubin I., Yarden Y. (2001). The basic biology of HER2. Ann Oncol.
4 Grunwald V., Hidalgo M. (2003). Developing inhibitors of the epidermal growth factor receptor for cancer treatment. J Natl Cancer Inst.
5 Mendelsohn J. (1990). Anti-epidermal growth factor receptor monoclonal antibodies as potential anti-cancer agents. J Steroid Biochem Mol Biol.
6 Yasui W., Sumiyoshi H., Hata J., Kameda T., Ochiai A., Ito H., Tahara E. (1988). Expression of epidermal growth factor receptor in human gastric and colonic carcinomas. Cancer Res.
7 Ang K.K., Berkey B.A., Tu X., Zhang H.Z., Katz R., Hammond E.H., Fu K.K., Milas L. (2002). Impact of epidermal growth factor receptor expression on survival and pattern of relapse in patients with advanced head and neck carcinoma. Cancer Res.
8 Costa S., Stamm H., Almendral A., Ludwig H., Wyss R., Fabbro D., Ernst A., Takahashi A., Eppenberger U. (1988). Predictive value of EGF receptor in breast cancer. Lancet.
9 Ethier S.P. (1995). Growth factor synthesis and human breast cancer progression. J Natl Cancer Inst.
10 Yarden Y. (2001). Biology of HER2 and its importance in breast cancer. Oncology.
11 Kim E.S., Khuri F.R., Herbst R.S. (2001). Epidermal growth factor receptor biology (IMC-C225). Curr Opin Oncol.
12 Cai W., Chen K., He L., Cao Q., Koong A., Chen X. (2007). Quantitative PET of EGFR expression in xenograft-bearing mice using 64Cu-labeled cetuximab, a chimeric anti-EGFR monoclonal antibody. Eur J Nucl Med Mol Imaging.
13 Schechter N.R., Yang D.J., Azhdarinia A., Kohanim S., Wendt R., Oh C.S., Hu M., Yu D.F., Bryant J., Ang K.K., Forster K.M., Kim E.E., Podoloff D.A. (2003). Assessment of epidermal growth factor receptor with 99mTc-ethylenedicysteine-C225 monoclonal antibody. Anticancer Drugs.
14 Wen X., Wu Q.P., Ke S., Ellis L., Charnsangavej C., Delpassand A.S., Wallace S., Li C. (2001). Conjugation with (111)In-DTPA-poly(ethylene glycol) improves imaging of anti-EGF receptor antibody C225. J Nucl Med.
15 Wang X., Zhu J., Zhao P., Jiao Y., Xu N., Grabinski T., Liu C., Miranti C.K., Fu T., Cao B.B. (2007). In vitro efficacy of immuno-chemotherapy with anti-EGFR human Fab-Taxol conjugate on A431 epidermoid carcinoma cells. Cancer Biol Ther.
16 Xu N., Cai G., Ye W., Wang X., Li Y., Zhao P., Zhang A., Zhang R., Cao B. (2009). Molecular imaging application of radioiodinated anti-EGFR human Fab to EGFR-overexpressing tumor xenografts. Anticancer Res.